# Anti-malondialdehyde-modified low-density lipoprotein MDA2 murine monoclonal antibody manganese-micelles

Chemical name: | Anti-malondialdehyde-modified low-density lipoprotein MDA2 murine monoclonal antibody manganese-micelles
Abbreviated name: | MDA2-Mn micelles
Synonym:
Agent category: | Antibody
Target: | Malondialdehyde-modified low-density lipoprotein (MDA-LDL)
Target category: | Antigen
Method of detection: | Magnetic resonance imaging (MRI)
Source of signal/contrast: | Gadolinium, Gd
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=44888831), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=217035086) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=ShowDetailView&TermToSearch=338) for more information about apolipoprotein B.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=MDA2)]

Magnetic resonance imaging (MRI) maps information about tissues spatially and functionally. Protons (hydrogen nuclei) are widely used in imaging because of their abundance in water molecules. Water comprises ~80% of most soft tissue. The contrast of proton MRI depends primarily on the density of the nucleus (proton spins), the relaxation times of the nuclear magnetization (T1, longitudinal; T2, transverse), the magnetic environment of the tissues, and the blood flow to the tissues. However, insufficient contrast between normal and diseased tissues requires the development of contrast agents. Most contrast agents affect the T1 and T2 relaxation times of the surrounding nuclei, mainly the protons of water. T2* is the spin–spin relaxation time composed of variations from molecular interactions and intrinsic magnetic heterogeneities of tissues in the magnetic field (1). Cross-linked iron oxide nanoparticles and other iron oxide formulations affect T2 primarily and lead to decreased signals. On the other hand, paramagnetic T1 agents, such as gadolinium (Gd^3+^) and manganese (Mn^2+^), accelerate T1 relaxation and lead to brighter contrast images.

Apolipoprotein E (apoE) is essential for the normal catabolism of triglyceride-rich lipoprotein chylomicrons (lipoprotein particles) (2). Oxidation of low-density lipoprotein (LDL) generates a number of highly reactive short chain-length aldehydic fragments of oxidized fatty acids capable of conjugating with lysine residues of apoliprotein B and other proteins. Oxidized LDL (OxLDL) is present in atherosclerotic lesions and is essential for the formation of foam cells in atherosclerotic plaques. During atherogenic conditions, deposition of lipids and extracellular matrix proteins on the endothelial cell surfaces of the aorta leads to the development of atherosclerotic plaques (3), which may erode and rupture. MDA2 is a murine monoclonal antibody to malondialdehyde-lysine epitopes of OxLDL and other oxidatively modified proteins, but not to normal LDL (4). The antibody-OxLDL complexes are taken up by macrophages and foam cells in the atherosclerotic plaques. Briley-Saebo et al. (5) demonstrated the accumulation of MDA2 micelles containing Gd (MDA2-Gd micelles (http://www.ncbi.nlm.nih.gov/books/NBK23013/)) in macrophages of atherosclerotic lesions in apoE-deficient (apoE^–/–^) mice using MRI. However, Gd may lead to renal toxicity in patients. In another study, Briley-Saebo et al. (6) demonstrated that MDA2-Mn micelles exhibited sensitive and robust in vivo detection of atherosclerotic lesions in apoE^–/–^ mice using MRI.

### Related Resource Links:

- Chapters in MICAD (MDA (http://www.ncbi.nlm.nih.gov/books?term=malondialdehyde%20AND%20micad%5Bbook%5D))
- Gene information in NCBI (apolipoprotein E (http://www.ncbi.nlm.nih.gov/gene/348))
- Articles in Online Mendelian Inheritance in Man (OMIM) (apolipoprotein E (http://omim.org/entry/107741))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=MDA2+synthesis)]

1,2-Distearoyl-sn-glycer-3-phosphoethanolamine-n-methoxy(polyethylene glycol-2000) ammonium salt (PEG-DSPE), Mn-DTPA-bis(stearyl-amid), and PEG-maleimide-DSPE were dissolved at a molar ratio of 49:50:1 in a chloroform:methanol solution with rhodamine added as a fluorescent label (6). The solvents were removed under heat and vacuum until a thin film was formed. The film was hydrated in a HEPES buffer (pH 7.0), and the sample was incubated at 65°C until micelles formed. MDA2 was modified with S-acetylthioglycolic acid N-hydroxysuccinimide ester and then covalently linked to the surface of the MDA2-Mn micelles. MDA2-Mn micelles have a hydrated diameter of 22 ± 2 nm with an r1 value of 9.3 nM^–1^s^–1^ at 60 MHz and 40ºC. The number of Mn molecules and the number of MDA2 monoclonal antibodies per MDA2-Mn micelle were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=MDA2+in+vitro)]

^125^I-MDA2 has been shown to bind specifically to human MDA-LDL but not to normal human LDL, high-density lipoprotein, very low-density lipoprotein, or bovine serum albumin (7). Confocal microscopy analysis showed that the highest accumulation of MDA2-Mn micelles in macrophages was obtained when both the macrophages and the MDA2-Mn micelles were pretreated with MDA-LDL; this accumulation was higher than with pretreatment of either one alone (5). The intracellular r1 value for MDA2-Mn micelles after incubation with J744a.1 macrophages (pretreated with MDA-LDL) was 45 ± 5 nM^–1^s^–1^, whereas the intracellular r1 value was not detectable in the macrophages incubated with untargeted Mn micelles (6).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=MDA2+rodentia)]

Briley-Saebo et al. (6) performed ex vivo biodistribution studies of MDA2-Mn micelles in 11-month-old apoE^–/–^ mice that were fed a high-fat, high-cholesterol diet at 6 weeks of age. Animals were injected with either 0.05 mmol Mn/kg MDA2-Mn micelles (n = 3 mice/group) or non-targeted Mn micelles (n = 3 mice/group). As a comparison, MDA2-Gd and non-targeted micelles (0.075 mmol Gd/kg) were also injected. The accumulation of Mn/Gd was determined as a percentage of injected dose (% ID) at 1, 2, 3, 4, and 7 d after injection. The blood half-life was 16.4 h for MDA2-Mn micelles and 3.4 h for non-targeted Mn micelles, whereas the blood half-life was 14.3 h for MDA2-Gd micelles and 1.5 h for non-targeted Gd micelles. Liver and kidney uptake of Mn peaked at 48 h with ~10% ID and 1% ID, respectively, and the liver and kidney accumulation levels of Gd were 40% ID and 2% ID, respectively. The atherosclerotic aorta showed 0.50%, 0.27%, and 0.12% ID of MDA2-Mn micelles at 24, 48, and 96 h, respectively. On the other hand, MDA2-Gd micelles exhibited accumulation values of 0.20%, 0.30%, and 0.22% ID Gd at 24, 48, and 96 h, respectively. Little Mn was detected in the aorta after injection of non-targeted Mn micelles. Sequential T1-weighted MRI images (9.4 T) showed that MDA2-Mn micelles caused increased atherosclerotic arterial vessel wall enhancement at 24–96 h after injection. The mean enhancement was 60%, 140%, 70%, 45%, and 10% at 1, 2, 3, 4, and 7 d, respectively. A similar enhancement was also observed with a human single-chain Fv antibody fragment IK17 targeted to MDA-like epitopes (IK17-Mn-micelles). On the other hand, MDA2-Gd micelles exhibited a gradual enhancement over time (50% at 1 d, 80% at 2 d, and 120% at 3 d and 4 d) with maximal enhancement (~150%) at 7 d. In contrast, non-targeted Mn micelles caused minimal signal enhancement of ~20% at these time points. Co-injection of excess MDA2 reduced the enhancement with MDA2-Mn micelles by >90% in the aorta at 48–96 h. Confocal microscopy revealed that MDA2 localized primarily with intraplaque foam cells/macrophages in atherosclerotic lesions of the arterial wall. Briley-Saebo et al. concluded that no significant difference in the MR efficacy was observed between the MDA2-Mn and MDA2-Gd micelles at the optimal imaging time points after injection (2 d vs.7 d, respectively).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=MDA2+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=MDA2+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=MDA2+human)]

No publication is currently available.

## NIH Support

R21 HL091399

## References

1 Wang Y.X., Hussain S.M., Krestin G.P. (2001). Superparamagnetic iron oxide contrast agents: physicochemical characteristics and applications in MR imaging. Eur Radiol.
2 Eichner J.E., Dunn S.T., Perveen G., Thompson D.M., Stewart K.E., Stroehla B.C. (2002). Apolipoprotein E polymorphism and cardiovascular disease: a HuGE review. Am J Epidemiol.
3 Libby P. (2002). Inflammation in atherosclerosis. Nature.
4 Palinski W., Yla-Herttuala S., Rosenfeld M.E., Butler S.W., Socher S.A., Parthasarathy S., Curtiss L.K., Witztum J.L. (1990). Antisera and monoclonal antibodies specific for epitopes generated during oxidative modification of low density lipoprotein. Arteriosclerosis.
5 Briley-Saebo K.C., Shaw P.X., Mulder W.J., Choi S.H., Vucic E., Aguinaldo J.G., Witztum J.L., Fuster V., Tsimikas S., Fayad Z.A. (2008). Targeted molecular probes for imaging atherosclerotic lesions with magnetic resonance using antibodies that recognize oxidation-specific epitopes. Circulation.
6 Briley-Saebo K.C., Nguyen T.H., Saeboe A.M., Cho Y.S., Ryu S.K., Volkava E., Dickson S., Leibundgut G., Weisner P., Green S., Casanada F., Miller Y.I., Shaw W., Witztum J.L., Fayad Z.A., Tsimikas S. (2012). In vivo detection of oxidation-specific epitopes in atherosclerotic lesions using biocompatible manganese molecular magnetic imaging probes. J Am Coll Cardiol.
7 Tsimikas S., Palinski W., Halpern S.E., Yeung D.W., Curtiss L.K., Witztum J.L. (1999). Radiolabeled MDA2, an oxidation-specific, monoclonal antibody, identifies native atherosclerotic lesions in vivo. J Nucl Cardiol.